# Fluorescein-conjugated cyclic decapeptides, CGLIIQKNEC (CLT1) and CNAGESSKNC (CLT2)

Chemical name: | Fluorescein-conjugated cyclic decapeptides, CGLIIQKNEC (CLT1) and CNAGESSKNC (CLT2)
Abbreviated name: | Fluorescent CLT peptides
Synonym: | Fluorescent CLT1, fluorescent CLT2
Agent Category: | Peptides
Target: | Clotted plasma proteins (fibrin and fibronectin)
Target Category: | Others (proteins)
Method of detection: | Optical imaging
Source of signal / contrast: | Fluorescein
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=tumor%20stroma%20and%20clotted%20plasma)]

Fluorescein-conjugated cyclic decapeptides, CGLIIQKNEC (CLT1) and CNAGESSKNC (CLT2), abbreviated as fluorescent CLT peptides, are two peptide agents that specifically home to tumors and wounds and are potentially useful for tumor-targeted imaging and therapy (1).

Tumor tissue is different from normal tissue in the content and function of its stroma. At the initial stage of tumor development, tumor cells secrete growth factors, including vascular permeability factor that renders the local microvasculature hyperpermeable to fibrinogen and other plasma proteins. Extravasated fibrinogen crosslinks with fibrin and other proteins, forming a meshwork in the tumor stroma (1, 2). This sequence also occurs in the process of wound-healing and in the progression of many other diseases, but the tumor stroma contains increased amounts of fibrinogen, collagen, fibronectin, fibrinogen-derived products, and other proteins (3). These proteins either come from the leaky blood vessels or are inappropriately synthesized by the tumor cells. Functionally, normal stroma generates an antiproliferative environment, whereas tumor stroma promotes tumor cell proliferation, migration, and lymphovascular invasion by providing adhesion proteins, proteases, and growth factors (2, 4).

Abnormal formation of clotted plasma protein meshwork in the tumor stroma and on the tumor blood vessel walls has prompted investigators to generate tumor stroma-targeted imaging and therapeutic agents. Pilch et al. screened a phage library on plasma clots and obtained two cyclic decapeptides (CLT; CLT1 and CLT2) (1). The fluorescence-labeled CLT peptides specifically accumulated in the fibrillar meshwork that existed in the tumor stroma, but they were not detectable in other tissues in animal models of human tumors. Ye et al. conjugated the CLT1 peptide with gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA), and the generated agent Gd-DTPA-CLT1 (http://www.ncbi.nlm.nih.gov/books/NBK23114/#Gd-DTPA-CLT1.Background) exhibited high specificity to the fibronectin-fibrin complexes in the tumor stroma (5). Simberg et al. also reported the clotted plasma protein-targeted multimodal agent CREKA-SPIO-Cy7 (http://www.ncbi.nlm.nih.gov/books/NBK23725/#CREKA-SPIO.Background), which was synthesized by conjugation of the peptide CREKA with superparamagnetic iron oxide and cyanine 7 (6). On the basis of the interaction between the fibrinogen-derived products and heparin, Yuk et al. synthesized the MRI contrast agent, Composite NPs, using heparin as the specific ligand (7, 8). Composite NPs have been shown to selectively distribute in tumors in an animal model of murine squamous cell carcinoma (7). This chapter summarizes the data obtained with the fluorescent CLT peptides (1).

### Related Resource Links:

Tumor stroma clotted plasma protein-targ (http://www.ncbi.nlm.nih.gov/books/?term=tumor%20stroma%20and%20clotted%20AND%20micad%5bbook%5d) e (http://www.ncbi.nlm.nih.gov/books/?term=tumor%20stroma%20and%20clotted%20AND%20micad%5bbook%5d) ted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=tumor%20stroma%20and%20clotted%20AND%20micad%5bbook%5d)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=16476999)]

CLT1 and CLT2 peptides were identified through screening of a phage library on clotted plasma (1). The phage selection was designed to amplify phages that bind to plasma clots but not to anticoagulated plasma. Three rounds of selection produced a pool of phages with seven-fold increased binding to plasma clots. Additional selection rounds did not increase the binding. Sequencing showed that the phages encoding the peptide inserts CLT1 and CLT2 were highly enriched among the clot-binding phages.

Peptides were then synthesized, conjugated to fluorescein isothiocyanate, and cyclized by exposure to air. A control peptide with the sequence of KAREC was also synthesized and labeled with fluorescein. The efficiency of fluorescein labeling was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=16476999)]

The CLT peptides, CLT1 and CLT2, exhibited three- to four-fold increased efficiency of binding to plasma clots compared to the control peptide. They did not significantly bind to clots made of purified fibrin or fibronectin immobilized on plastic (results not shown). These results indicate that the two peptides specifically bind to clots containing fibrin and fibronectin (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=16476999)]

Pilch et al. tested the homing of CLT1 and CLT2 in tumors produced in BALB/c nu/nu mice, mouse mammary tumor virus (MMTV) PyMT mice, fibrinogen knockout mice, and transgenic plasma fibronectin-deficient C57BL/6-Fn(fl/fl)Mx-Cre^+^ mice and their wild-type littermates (1). The MMTV-PyMT mice develop breast cancer under the influence of a polyoma middle T antigen driven by the mouse tumor virus promoter. Imaging of the whole tissues ex vivo was performed with a Leica fluorescence stereomicroscope at 3 h after the peptide injection.

BALB/c nu/nu mice bearing orthotopic MDA-MB-435 xenograft tumors (human breast cancer) were intravenously injected with fluorescent CLT1 (n = 6), CLT2 (n = 4), or the control peptide (n = 4). Intense fluorescence was observed in the tumors from the mice injected with CLT1 and CLT2, but not in the tumors from the mice injected with the control peptide. No fluorescence was observed in healthy organs of the CLT-injected animals. Microscopy showed that the fluorescence from the CLT peptides and the fluorescence from the fibrin staining colocalized in tumor sections. CLT peptides also co-distributed with fibronectin (data not shown). The co-distribution results of the CLT peptides, fibrin, and fibronectin in the MMTV-PyMT transgenic breast tumors were identical to those obtained with the MDA-MB-435 xenografts (data not shown). These results suggest that CLT peptides are associated with the fibrin and fibronectin in tumor stroma.

Fibrinogen knockout mice bearing B16-F1 tumors (mouse melanoma) were used to study the role of fibrin, fibrinogen, and fibronectin in the homing of the CLT peptides to tumors. The CLT peptides homed to B16-F1 tumors grown in the wild-type C57BL/6 mice (n = 10), which produce a fibrillar meshwork. In contrast, only faint, evenly distributed fluorescence was observed in tumors (n = 4) grown in the fibrinogen knockout mice, which lack the ability to produce fibrin. In plasma fibronectin-deficient mice, B16-F1 tumors grown in wild-type littermates also accumulated CLT peptides in the fibrillar matrix, but mice lacking plasma fibronectin did not (n = 6 mice). Unlike in the model of fibrinogen knockout mice, there was no residual peptide binding to the tumors in the model of plasma fibronectin-deficient mice. These results suggest that both fibrin and fibronectin from plasma are needed for the homing of CLT peptides in tumors.

CLT peptide homing to injured tissue was tested in mice with wire injury of the femoral artery and in mice with skin incisions (1). Fluorescent CLT peptides homed to the de-endothelialized femoral arteries (n = 5), producing strong fluorescence in the vessel wall. CLT homing was also seen in crush injuries of the muscle (n = 3) and in skin wounds resulting from incisions (n = 4). No CLT peptide homing was observed in intact arteries, muscles, skin, or other healthy tissues of the mice with injuries. The control peptide showed no homing to the injured tissues (data not shown) suggesting the specificity of CLT peptides.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
2 Simpson-Haidaris P.J., Rybarczyk B. (2001). Tumors and fibrinogen. The role of fibrinogen as an extracellular matrix protein. Ann N Y Acad Sci.
3 Rybarczyk B.J., Lawrence S.O., Simpson-Haidaris P.J. (2003). Matrix-fibrinogen enhances wound closure by increasing both cell proliferation and migration. Blood.
4 Malik G., Knowles L.M., Dhir R., Xu S., Yang S., Ruoslahti E., Pilch J. (2010). Plasma fibronectin promotes lung metastasis by contributions to fibrin clots and tumor cell invasion. Cancer Res.
5 Ye F., Wu X., Jeong E.K., Jia Z., Yang T., Parker D., Lu Z.R. (2008). A peptide targeted contrast agent specific to fibrin-fibronectin complexes for cancer molecular imaging with MRI. Bioconjug Chem.
6 Simberg D., Duza T., Park J.H., Essler M., Pilch J., Zhang L., Derfus A.M., Yang M., Hoffman R.M., Bhatia S., Sailor M.J., Ruoslahti E. (2007). Biomimetic amplification of nanoparticle homing to tumors. Proc Natl Acad Sci U S A.
7 Yuk S.H., Oh K.S., Cho S.H., Lee B.S., Kim S.Y., Kwak B.K., Kim K., Kwon I.C. (2011). Glycol chitosan/heparin immobilized iron oxide nanoparticles with a tumor-targeting characteristic for magnetic resonance imaging. Biomacromolecules.
8 Norrby K. (2006). Low-molecular-weight heparins and angiogenesis. APMIS.